# Cy7-Tetrameric arginine-glycine-aspartic acid peptide

Chemical name: | Cy7-Tetrameric arginine-glycine-aspartic acid peptide
Abbreviated name: | Cy7-E{E[c(RGDyK)]_2_}_2_
Synonym: | Cy7-Tetrameric RGD peptide
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal/contrast: | Indocyanine 7 (Cy7)
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cy7-tetrameric%20RGD%29%20OR%20%28fluorescence%20imaging%20of%20RGD%29)]

Indocyanine 7 (Cy7)–tetrameric arginine-glycine-aspartic acid peptide (Cy7 E{E[c(RGDyK)]_2_}_2_) is an integrin-targeted molecular imaging agent developed for near-infrared (NIR) fluorescence imaging of tumor vasculature and tumor angiogenesis (1). Cy7 has a peak excitation wavelength of 743 nm and a peak emission wavelength of 767 nm.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiologic processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue, but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature. Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7).

Various RGD peptides in both linear and cyclic forms have been developed for in vivo binding to integrin α_v_β_3_ (8). It has been hypothesized that cyclic RGD peptide may have a faster rate of receptor binding or a slower rate of dissociation from the integrin α_v_β_3_ than linear single RGD peptides (9). Wu et al. (9) proposed to evaluated whether a multimeric RGD peptide with >2 repeating cyclic RGD units would further enhance the affinity of the receptor-ligand interactions through a polyvalency effect. They also suggested that the increase in molecular size might prolong circulation time and reduce tumor washout rate. Optical imaging is an imaging method that utilizes light photons emitted from bioluminescence and fluorescence probes (7). Depth penetration is one major limiting factor in in vivo optical imaging. Currently, in vivo optical imaging has wide applications in small animal imaging but only limited applications in large animal and human studies (10). NIR fluorescence imaging (light range, 650−900 nm) has the advantages of relatively higher tissue penetration and lower autofluorescence from nontarget tissue. NIR fluorescent dyes conjugated RGD peptides such as Cy5.5-c(RGDyK), Cy5.5-c(RGDfK), and Cyp-GRD have been shown to visualize subcutaneously implanted integrin α_v_β_3_−positive tumors (11-14). Wu et al. (1) investigated the use of the NIR fluorescent dye Cy7−conjugated tetrameric RGD to detect tumor integrin expression. Cy7 was chosen because of its deeper tissue penetration, lower scattering effect, and lower background autofluorescence compared to Cy5.5. The polyvalency effect and suitable apparent size of Cy7-E{E[c(RGDyK)]_2_}_2_ appeared to make it a highly potent integrin α_v_β_3_ probe.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Cy7-tetrameric%20RGD%29%20OR%20%28fluorescence%20imaging%20of%20RGD%29%29%20AND%20synthesis)]

Wu et al. (1) reported the synthesis of Cy7-E{E[c(RGDyK)]_2_}_2_ by using the monomeric cyclic RGD as the basic building block. Briefly, the fully protected linear pentapeptide H-D-Tyr(OtBu)-Lys(Boc)-Arg(Pbf)-Gly-Asp(OtBu)-OH was cleaved from the resin without affecting the side-chain protecting groups (15). Head-to-tail cyclization was then carried out in N,N-dimethylformamide. All side-chain protecting groups were then removed by treatment with trifluoroacetic acid (TFA) at room temperature for 1 h. The resulting c(RGDyK) was purified by high-performance liquid chromatography (HPLC). In the preparation of the tetrameric E{E[c(RGDyK)]_2_}_2_, Boc-Glu(OSu)-OSu was first prepared by mixing Boc-protected glutamic acid in N,N-dimethylformamide with N-hydroxysuccinimide and dicyclohexylcarbodiimide. The mixture was stirred at room temperature for 10 h. Boc-Glu(OSu)-OSu was obtained after this mixture was filtered to remove the dicyclohexylurea byproduct. c(RGDyK) was added to Boc-Glu(OSu)-OSu in N,N-dimethylformamide, and the pH was adjusted to 8.5. The mixture was stirred at room temperature overnight, and the Boc group was removed by TFA treatment to produce the dimeric E[c(RGDyK)]_2_ with a 95% yield. This procedure was repeated with E[c(RGDyK)]_2_ to produce the tetrameric E{E[c(RGDyK)]_2_}_2_ with a 92% yield.

Cy7-E{E[c(RGDyK)]_2_}_2_ conjugate was synthesized by conjugation of monofunctional hydroxysuccinimide of Cy7 (Cy7-NHS) with the α-amino group of glutamine residue (1). In this reaction, E{E[c(RGDyK)]_2_}_2_ in sodium borate buffer (pH 8.5) was mixed with Cy7-NHS in water at 4ºC. The reaction vessel was allowed to warm up to room temperature. TFA was added after 2 h of reaction, and the preparation was purified by HPLC to yield Cy7-E{E[c(RGDyK)]_2_}_2_. The Cy7-E{E[c(RGDyK)]_2_}_2_ conjugate was identified by matrix-assisted laser desorption/ionization–time-of-flight mass spectroscopy (MALDI-TOF) with a calculated molecular mass of 3,431.5 kDa.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Cy7-tetrameric%20RGD%29%20OR%20%28fluorescence%20imaging%20of%20RGD%29%29%20AND%20in%20vitro)]

The spectral properties of unconjugated Cy7 were reported to be 747 nm absorption maxima, 774 nm emission maxima, 0.28 quantum yield, and 200,000 M−^1^cm−^1^ molar extinction coefficient (16, 17). The ultraviolet absorption and emission spectra of Cy7-E{E[c(RGDyK)]_2_}_2_ were similar to that of unconjugated Cy7 in aqueous solution (1). No significant change in quantum yield was observed.

In vitro receptor binding assays of Cy7-E{E[c(RGDyK)]_2_}_2_ with integrin-positive U87MG cells and ^125^I-echistatin, an integrin-specific radioligand, gave an inhibition concentration value (IC_50_) of 23.1 ± 2.5 nM (n = 3) (1). In comparison, the IC_50_ values for the Cy7-c(RGDyK) monomer and the Cy7-E[c(RGDyK)]_2_ dimer were 70.1 ± 5.3 nM and 28.2 ± 2.8 nM, respectively. Cy7 conjugation appeared to cause minimal disturbance to receptor affinity. In comparison, the IC_50_ values of fluorobenzoyl-c(RGDyK) and fluorobenzoyl-E[c(RGDyK)]_2_ were reported to be 6.7 ± 0.5 nM and 3.5 ± 0.3 nM, respectively (18). Similar results were observed with U87AMG cell-staining studies. Only a weak signal was detected when the cells were incubated with the unconjugated Cy7. The fluorescence intensity of the stained cells followed the order of Cy7-E{E[c(RGDyK)]_2_}_2_ > Cy7-E[c(RGDyK)]_2_ > Cy7-c(RGDyK)_._

Serum stability studies of incubating Cy7-E{E[c(RGDyK)]_2_}_2_ at 37ºC in complete mouse serum indicated that the Cy7 conjugate remained stable for 24 h (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Cy7-tetrameric%20RGD%29%20OR%20%28fluorescence%20imaging%20of%20RGD%29%29%20AND%20rodentia)]

Wu et al. (1) conducted NIR fluorescence imaging of tumor integrin α_v_β_3_ in mice bearing subcutaneous U87MG tumor. Each mouse received a dose of 500 pmol of Cy7-E{E[c(RGDyK)]_2_}_2_. Fluorescence signal was clearly visualized in the tumor as early as 30 min. The fluorescence intensity in the tumor reached early maxima and slowly washed out. The tumor/normal tissue ratio (T/N) quantified by region of interest peaked at 2 h with a value of 4.35 ± 0.26 (n = 3). In comparison, the T/N ratios for Cy7-c(RGDyK) and Cy7-E[c(RGDyK)]_2_ were 2.50 ± 0.15 and 2.72 ± 0.08, respectively. The kidneys were also visualized as because of renal clearance. Fluorescence signal intensities also originated in the liver and gastrointestinal tracts. Coinjection of 200 μg unconjugated c(RGDyK) per mouse reduced the T/N ratio of Cy7-E{E[c(RGDyK)]_2_}_2_ at 2 h to 1.95 ± 0.02.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Cy7-tetrameric%20RGD%29%20OR%20%28fluorescence%20imaging%20of%20RGD%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Cy7-tetrameric%20RGD%29%20OR%20%28fluorescence%20imaging%20of%20RGD%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Cy7-tetrameric%20RGD%29%20OR%20%28fluorescence%20imaging%20of%20RGD%29%29%20AND%20human)]

No publication is currently available.

## NIH Support

NCI R21 CA102123, NIBIB R21 EB001785, NCI SAIRP R24 CA93862, ICMIC P50 CA114747, NCI CCNE US4.

## References

1 Wu Y., Cai W., Chen X. (2006). Near-infrared fluorescence imaging of tumor integrin alpha v beta 3 expression with Cy7-labeled RGD multimers. Mol Imaging Biol.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Wu Y., Zhang X., Xiong Z., Cheng Z., Fisher D.R., Liu S., Gambhir S.S., Chen X. (2005). microPET imaging of glioma integrin {alpha}v{beta}3 expression using (64)Cu-labeled tetrameric RGD peptide. J Nucl Med.
10 Bremer C., Ntziachristos V., Weissleder R. (2003). Optical-based molecular imaging: contrast agents and potential medical applications. Eur Radiol.
11 Wang W., Ke S., Wu Q., Charnsangavej C., Gurfinkel M., Gelovani J.G., Abbruzzese J.L., Sevick-Muraca E.M., Li C. (2004). Near-infrared optical imaging of integrin alphavbeta3 in human tumor xenografts. Mol Imaging.
12 Kwon S., Ke S., Houston J.P., Wang W., Wu Q., Li C., Sevick-Muraca E.M. (2005). Imaging dose-dependent pharmacokinetics of an RGD-fluorescent dye conjugate targeted to alpha v beta 3 receptor expressed in Kaposi's sarcoma. Mol Imaging.
13 Achilefu S., Bloch S., Markiewicz M.A., Zhong T., Ye Y., Dorshow R.B., Chance B., Liang K. (2005). Synergistic effects of light-emitting probes and peptides for targeting and monitoring integrin expression. Proc Natl Acad Sci U S A.
14 Chen X., Conti P.S., Moats R.A. (2004). In vivo near-infrared fluorescence imaging of integrin alphavbeta3 in brain tumor xenografts. Cancer Res.
15 Chen X., Park R., Shahinian A.H., Bading J.R., Conti P.S. (2004). Pharmacokinetics and tumor retention of 125I-labeled RGD peptide are improved by PEGylation. Nucl Med Biol.
16 Law B., Curino A., Bugge T.H., Weissleder R., Tung C.H. (2004). Design, synthesis, and characterization of urokinase plasminogen-activator-sensitive near-infrared reporter. Chem Biol.
17 (2003). 18-1171-47 AA, Amersham Biosciences. p. 1-8.
18 Chen X., Tohme M., Park R., Hou Y., Bading J.R., Conti P.S. (2004). Micro-PET imaging of alphavbeta3-integrin expression with 18F-labeled dimeric RGD peptide. Mol Imaging.